# Cys-Arg-Lys-Arg-Leu-Asp-Arg-Asn-Cys-glycol chitosan-Cy5.5 nanoparticles

Chemical name: | Cys-Arg-Lys-Arg-Leu-Asp-Arg-Asn-Cys-glycol chitosan-Cy5.5 nanoparticles
Abbreviated name: | AP-HGC-Cy5.5 NPs
Synonym:
Agent category: | Peptide
Target: | Interleukin-4 receptor (IL-4R)
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal/contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AP-HGC%20Cy5.5)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals.

Endothelial cells are important cells in inflammatory responses (3, 4). Bacterial lipopolysaccharide, virus, inflammation, and tissue injury increase the secretion of tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokines and chemokines. Emigration of leukocytes from blood is dependent on their ability to adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1, vascular cell adhesion molecule-1, integrins, and selectins. Chemokines are chemotactic to leukocytes toward sites of inflammation and tissue injury. During atherogenic conditions, lipid deposits on the endothelial cell surfaces of aorta and inflammatory cells lead to development of atherosclerotic plaques (5), which may erode and rupture.

Interleukin-4 (IL-4) is a lymphokine capable of inducing T and B cell differentiation (6). IL-4 receptor (IL-4R) is also found on endothelial cells, macrophages, and smooth muscle cells of atherosclerotic plaques (7). The atherosclerotic plaque-homing peptide (AP) Cys-Arg-Lys-Arg-Leu-Asp-Arg-Asn-Cys (CRKRLDRNC) has been identified using phage display screening (7). Park et al. (8) prepared Cy5.5- and AP-tagged nanoparticles (NPs) using hydrophobically modified glycol chitosan (HGC) for use in imaging atherosclerotic plaques. Cy5.5 is a NIR fluorescent dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AP-HGC%20Cy5.5+synthesis)]

Glycol chitosan (47 kDa) and 5β-cholanic acid (0.056 mole per 1 mole of sugar residues) in the presence of 1-ethyl-3-(3-dimethylaminopropyl)-carbodiimide hydrochloride and N-hydroxysuccinimide ester (NHS) were incubated for 24 h (8). The resulting product, HGC, was purified with dialysis. AP was conjugated to HGC by incubation with N-succinimidyl 4-(maleimidomethyl)cyclohexane carboxylate in 1:10 molar ratio. Cy5.5-NHS was used to conjugate AP-HGC to form AP-HGC-Cy5.5 NPs. There are 4.7 5β-cholanic acid molecules, 13 AP peptides, and 1.7 Cy5.5 molecules per NP. The average size of AP-HGC-Cy5.5 NPs in water as measured with dynamic light scattering was 314 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AP-HGC%20Cy5.5+in+vitro)]

In vitro binding tests showed that binding of AP-HGC-Cy5.5 NPs (100 µg/ml) to bovine arterial endothelial cells (BAECs) expressing IL-4R was induced with TNFα (8). There was a one-fold increase in fluorescence intensity over control BAECs and TNFα-activated BAECs+HGC-Cy5.5 NPs after 1–2 h of incubation. Confocal microscopy showed that most of the AP-HGC-Cy5.5 NPs bound to the cell membranes of activated BAECs. Shear flow experiments showed that AP-HGC-Cy5.5 NPs bound to activated BAECs but not to non-activated BAECs. HGC-Cy5.5 NPs, without the targeting peptide AP, showed no binding to activated BAECs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AP-HGC%20Cy5.5+rodentia)]

Park et al. (8) performed fluorescence imaging of the aortic arch of three normal mice and three low-density lipoprotein receptor-deficient (Ldlr^-/-^) mice after intravenous injection of AP-HGC-Cy5.5 NPs (5 mg/kg). The fluorescence photon counts were 7,800 and 23,500 from the aortic arch of normal and Ldlr^-/-^ mice at 6 h after injection, respectively. The fluorescence signal colocalized with lipid deposits at the aortic arch of Ldlr^-/-^ mice. The AP-HGC-Cy5.5 NPs bound to the luminal surface of the atherosclerotic lesions as well as inside the lesions. Little accumulation of AP-HGC-Cy5.5 NPs was observed in the aortic arch of normal mice. Neither blocking experiment nor use of the control HGC-Cy5.5 NPS was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AP-HGC%20Cy5.5+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AP-HGC%20Cy5.5+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AP-HGC%20Cy5.5+human)]

No publication is currently available.

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
4 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
5 Libby P., Ridker P.M., Maseri A. (2002). Inflammation and atherosclerosis. Circulation.
6 Nelms K., Keegan A.D., Zamorano J., Ryan J.J., Paul W.E. (1999). The IL-4 receptor: signaling mechanisms and biologic functions. Annu Rev Immunol.
7 Hong H.Y., Lee H.Y., Kwak W., Yoo J., Na M.H., So I.S., Kwon T.H., Park H.S., Huh S., Oh G.T., Kwon I.C., Kim I.S., Lee B.H. (2008). Phage display selection of peptides that home to atherosclerotic plaques: IL-4 receptor as a candidate target in atherosclerosis. J Cell Mol Med.
8 Park K., Hong H.Y., Moon H.J., Lee B.H., Kim I.S., Kwon I.C., Rhee K. (2008). A new atherosclerotic lesion probe based on hydrophobically modified chitosan nanoparticles functionalized by the atherosclerotic plaque targeted peptides. J Control Release.